# [^111^In]5-[(3aR,6S,6aS)-2-Oxo-1,3,3a,4,6,6a-hexahydrothieno[3,4-d]imidazol-6-yl]pentanoic acid

Chemical name: | [^111^In]5-[(3aR,6S,6aS)-2-Oxo-1,3,3a,4,6,6a-hexahydrothieno[3,4-d]imidazol-6-yl]pentanoic acid
Abbreviated name: | [^111^In]Biotin
Synonym:
Agent Category: | Compound
Target: | Streptavidin/avidin
Target Category: | Ligand-receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of Signal/Contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+Biotin)]

White blood cells (WBCs) labeled with radioactive gallium (^67^Ga), indium (^111^In), or technetium (^99m^Tc) are often used for the detection of infections, but this application of WBCs is laborious and requires the use of autologous WBCs, which increases the probability of introducing an infection (1). In addition, this technique may not detect all types of infections. Although computed tomography (CT) and magnetic resonance imaging (MRI) are often used to characterize an infection or inflammation, these techniques also have limitations. CT cannot be used at frequent intervals because it requires the use of high radiation doses, and MRI has a low sensitivity to detect infections during early stages until major pathological changes occur (2). Polyclonal immunoglobulins and albumin labeled with ^67^Ga, or ^111^In, or ^99m^Tc have also been used for the detection of infections and inflammation, but these proteins clear very slowly from circulation, tend to accumulate in the liver, and are not suitable for the early detection of infection or inflammation (3).

The technique of pretargeting with a bifunctional antibody followed by the administration of an appropriate radiolabeled ligand was used successfully to image tumors in mice (4). Rusckowski et al. used a similar approach for the detection of infection and administered ^111^In-labeled biotin to animals a few hours after pretreatment with unlabeled streptavidin, a 65-kDa protein (5). Streptavidin is assumed to accumulate at the site of infection/inflammation because of increased vascularity and vascular permeability. Subsequent administration of ^111^In-biotin leads to the accumulation of radioactivity at the site of infection or inflammation because biotin has a very strong affinity (dissociation constant = 10^-15^) for streptavidin (6). Free ^111^In-biotin is secreted through the kidneys, whereas a complex of ^111^In-biotin and streptavidin not bound at the site of infection or inflammation is secreted through the hepatobiliary system (6). This technique was used successfully for the detection of infections after prosthetic vascular graft (3, 7) and osteomyelitis (8), including that of the vertebra (9).

Although the components used to prepare ^111^In-biotin and perform this work in humans are available commercially, Lazzeri et al. have stated that the technique is not approved for this indication by the United States Food and Drug Administration (9). It is pertinent to mention streptavidin and avidin are both targets of biotin. Streptavidin is produced by Streptomyces avidinii whereas avidin is found in avian eggs, but both have been used for the detection of infections (see sections below).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+biotin+synthesis)]

^111^In-Labeled biotin derivatives were initially prepared by Virzi et al. (10). They have also detailed the synthesis of the respective diethylenetriamine pentaacetic acid (DTPA) and ethylene diamine tetraacetic acid (EDTA) derivatives of biotin (10). The two derivatives were labeled with ^111^In in 0.5 M sodium acetate buffer (pH 6.0) to a specific activity of up to 125 mCi/1.2 μmol (4,625 MBq/1.2 μmol). Serum stability of the labeled derivatives was determined by incubating the conjugates with avidin-agarose beads in human serum at 37°C for 24 h with vigorous shaking. The beads were then recovered and washed so the amount of bound radioactivity could be determined. Approximately 95% of the radioactivity was reported to remain bound to the beads, indicating that the avidin-biotin complex was relatively stable under the experimental conditions used (10).

The synthesis of ^111^In-biotin was also described by Lazzeri et al. (9). Briefly, DTPA-conjugated biotin was purchased commercially and diluted in 0.05 M acetate buffer (pH 5.5). Aliquots of DTPA-biotin were stored at 4°C until required for labeling. Just before use, the DTPA-biotin was mixed with radioactive indium chloride ([^111^In]Cl), and the mixture was incubated at room temperature for 15 min. Labeling efficiency of the reaction was reported to be >98% as determined with instant thin-layer chromatography (5, 11). The specific activity, purity, and stability of the radiochemical were not reported (5, 9, 11).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+biotin+in+vitro+studies)]

Virzi et al. investigated the accumulation of the respectively ^111^In-labeled DTPA and EDTA derivatives in two tumor cell lines, H-MESO and LS-174T (10). Compared with the EDTA derivative, a higher amount of the DTPA derivative was reported to accumulate in the two tumor cell types (P value varied between 0.1 and 0.001, depending on the derivative; see Virzi et al. for details (10)). In another study with H-MESO cells, the investigators showed that the accumulation of the ^111^In-labeled DTPA-biotin derivative was not energy- or receptor-dependent and was as a result of passive diffusion (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+biotin+rodentia)]

The accumulation and biodistribution of the ^111^In-labeled derivatives of DTPA and EDTA were respectively investigated in normal mice (n = 6 animals/biotin derivative) with avidin-agarose beads implanted in the left thigh (10). The animals were imaged 2 h after administration of the radioactivity and 1 day after injection of avidin-agarose beads. All the animals were killed 24 h after injection of the radiolabels, and various tissues were counted for radioactivity. Between the two derivatives, ^111^In-labeled EDTA-biotin was reported to be superior to the DTPA derivative (10). The ratio of ^111^In accumulated in the avidin-agarose beads in the left thigh to the ^111^In accumulated in the other tissue was consistently higher with the EDTA derivative (varying from 11 to 340) compared with the same ratio with the DTPA derivative (ratio varied from 0.5 to 15). Both labeled derivatives (n = 2 animals per derivative) were reported to accumulate in the avidin-agarose beads when imaged 2 h after injection of the label. Compared with ^111^In-DTPA, only the ^111^In-labeled DTPA-biotin was shown to accumulate in the H-MESO tumor cells implanted into the peritoneal cavity of nude mice.

In another study, imaging of an Escherichia coli infection in the thigh of mice with ^111^In-labeled polyclonal non-specific IgG was compared with animals pretargeted with streptavidin followed by injection with ^111^In-labeled biotin (5). In this study the stability of the ^111^In-labeled DTPA derivative was shown to be superior to that of the ^111^In-labeled EDTA derivative under in vitro conditions (5). In this study mice with the infection were pretargeted with streptavidin (n = 4–6 animals) and injected intraperitoneally with ^111^In-labeled EDTA-biotin. Control animals received either ^111^In-IgG or ^111^In-strepavidin or ^111^In-labeled EDTA-biotin alone. Subsequently, the animals treated with streptavidin and ^111^In-labeled EDTA-biotin were shown to have high infected thigh-to-normal tissue ratios. Pretreatment of animals with streptavidin followed by injecting the radioactivity and imaging after 3 h showed there was a higher accumulation of radioactivity at the sites of infection compared to the accumulation observed in animals treated with radiolabeled IgG or streptavidin alone (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+biotin+humans)]

Chiesa et al evaluated the use of avidin and ^111^In-labeled DTPA-biotin for localizing vascular graft infection in 26 patients (3). From this group, 16 patients had various prosthetic grafts (group A), and the remaining 10 patients served as controls (group B). Patients from both groups were injected with avidin, and 24 h later they were treated with ^111^In-labeled DTPA-biotin. Whole-body imaging was performed 10 min and 2 h after administration. Scan results were compared with traditional imaging modalities and clinical outcome for the patients. In group A, three grafts (2 patients) were excluded from the study; in addition, there were 6 true-positives, 1 false-positive, and 11 true-negatives, and in group B there were 10 true-negatives. The overall sensitivity of the technique was reported to be 100%, with a specificity of 95%, an accuracy of 96%, a positive predictive value of 86%, and a negative predictive value of 100%. From this study the investigators concluded that avidin/^111^In-labeled DTPA-biotin scintigraphy could be used as a non-invasive method for the detection of prosthetic vascular graft infections (3). Using the same technique, Samuel et al. reached a similar conclusion with 25 patients with various types of grafts (total 29 grafts) (7).

Rusckowski et al. used the two-step streptavidin/^111^In-biotin protocol for a preliminary imaging study of chronic osteomyelitis in 15 patients (12). The patients were administered streptavidin and 24 h later were given ^111^In-labeled EDTA-biotin. On another occasion, 5 patients received ^111^In-labeled EDTA-biotin alone (without the pre-administration of streptavidin), and as another control 7 of the 15 patients were separately imaged after the administration of ^111^In-IgG alone. Accumulation of radioactivity in focal areas was identified in all patients pretreated with streptavidin within 10 min of administration of labeled biotin, and retention of the label was evident up to 24 h later. Similar areas of radioactivity accumulation were also observed when only labeled biotin was administered (12). Similar accumulation of radioactivity was also observed with ^111^In-labeled IgG, but with a delayed timing. The investigators concluded that the two-step streptavidin/^111^In-labeled EDTA-biotin protocol may be a suitable alternative to ^111^In-IgG for the detection of infection.

Lazzeri et al. compared the avidin/^111^In-labeled DTPA-biotin imaging approach with the use of leukocytes labeled with hexamethylpropylene amine oxime labeled with radioactive technetium (^99m^Tc-HMPAO) for the imaging of infection/inflammation in 54 patients with skeletal lesions (8). Avidin was administered as an intravenous bolus, and ^111^In-labeled DTPA-biotin was injected after 4 h. Imaging was acquired 30 min and 16–18 h after the administration of ^111^In-labeled DTPA-biotin. Among these patients, ^99m^Tc-HMPAO was used with 39 patients. The overall sensitivity of the avidin/^111^In-labeled DTPA-biotin scan was reported to be 97.7% versus 88.9% with ^99m^Tc-HMPAO. In general, there was no particular advantage for the use of avidin/^111^In-labeled DTPA-biotin compared to ^99m^Tc-HMPAO; however, the lower number of manipulations involved with avidin/^111^In-labeled DTPA-biotin imaging is considered to be an advantage over leukocytes labeled with ^99m^Tc-HMPAO because these cells can be easily contaminated during separation and rediolabeling (8).

In another study from the same laboratory, the use of streptavidin/^111^In-labeled DTPA-biotin scintigraphy in 55 patients with suspected vertebral osteomyelitis was compared with MRI (n = 32 patients) and CT (n = 24 patients) (6). The patients were infused with streptavidin, and ^111^In-labeled DTPA-biotin was administered 4 h later, followed by imaging after 60 min. Streptavidin/^111^In-labeled DTPA-biotin scintigraphy had a sensitivity of 94% and a specificity of 95%. The corresponding sensitivity values were reported to be 54% and 35% with a specificity of 75% and 57% for MRI and CT, respectively. This clearly indicated that the method with streptavidin/^111^In-labeled DTPA-biotin scintigraphy was superior to either MRI or CT for the detection of vertebral osteomyelitis (6).

On the basis of earlier observations (11, 12) that radioactively labeled biotin can be used for the detection of infections, Lazzeri evaluated the use of ^111^In-labeled DTPA-biotin alone for the imaging of vertebral osteomyelitis in 110 patients (9). Among these patients, 71 individuals were suspected to have a hematogenous vertebral infection (group 1), and 39 patients were suspected to have a postsurgical infection (group 2). The final diagnosis was performed with bacterial cultures, histopathological analysis, and/or clinical/imaging follow-up for at least 1 year. Scintigraphy with ^111^In-labeled DTPA-biotin alone was reported to have a sensitivity of 84% and a specificity of 98% for patients in group 1, and the sensitivity and specificity were 100% and 84% for the patients in group 2. The investigators concluded that ^111^In-labeled DTPA-biotin scintigraphy had a high accuracy for the detection of infections.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the studies presented in this chapter were supported by NIH grants CA 33029, AI 25570, and RFP NCI-CM-97570.

## References

1 Kumar R., Basu S., Torigian D., Anand V., Zhuang H., Alavi A. (2008). Role of modern imaging techniques for diagnosis of infection in the era of 18F-fluorodeoxyglucose positron emission tomography. Clin Microbiol Rev.
2 Alavi A., Lakhani P., Mavi A., Kung J.W., Zhuang H. (2004). PET: a revolution in medical imaging. Radiol Clin North Am.
3 Chiesa R., Melissano G., Castellano R., Fernandez Zamora C., Astore D., Samuel A., Paganelli G., Fazio F., Grossi A. (1995). Avidin and 111In-labelled biotin scan: a new radioisotopic method for localising vascular graft infection. Eur J Vasc Endovasc Surg.
4 Goodwin D.A., Meares C.F., McCall M.J., McTigue M., Chaovapong W. (1988). Pre-targeted immunoscintigraphy of murine tumors with indium-111-labeled bifunctional haptens. J Nucl Med.
5 Rusckowski M., Fritz B., Hnatowich D.J. (1992). Localization of infection using streptavidin and biotin: an alternative to nonspecific polyclonal immunoglobulin. J Nucl Med.
6 Lazzeri E., Pauwels E.K., Erba P.A., Volterrani D., Manca M., Bodei L., Trippi D., Bottoni A., Cristofani R., Consoli V., Palestro C.J., Mariani G. (2004). Clinical feasibility of two-step streptavidin/111In-biotin scintigraphy in patients with suspected vertebral osteomyelitis. Eur J Nucl Med Mol Imaging.
7 Samuel A., Paganelli G., Chiesa R., Sudati F., Calvitto M., Melissano G., Grossi A., Fazio F. (1996). Detection of prosthetic vascular graft infection using avidin/indium-111-biotin scintigraphy. J Nucl Med.
8 Lazzeri E., Manca M., Molea N., Marchetti S., Consoli V., Bodei L., Bianchi R., Chinol M., Paganelli G., Mariani G. (1999). Clinical validation of the avidin/indium-111 biotin approach for imaging infection/inflammation in orthopaedic patients. Eur J Nucl Med.
9 Lazzeri E., Erba P., Perri M., Tascini C., Doria R., Giorgetti J., Mariani G. (2008). Scintigraphic imaging of vertebral osteomyelitis with 111in-biotin. Spine.
10 Virzi F., Fritz B., Rusckowski M., Gionet M., Misra H., Hnatowich D.J. (1991). New indium-111 labeled biotin derivatives for improved immunotargeting. Int J Rad Appl Instrum B.
11 Shoup T.M., Fischman A.J., Jaywook S., Babich J.W., Strauss H.W., Elmaleh D.R. (1994). Synthesis of fluorine-18-labeled biotin derivatives: biodistribution and infection localization. J Nucl Med.
12 Rusckowski M., Paganelli G., Hnatowich D.J., Magnani P., Virzi F., Fogarasi M., DiLeo C., Sudati F., Fazio F. (1996). Imaging osteomyelitis with streptavidin and indium-111-labeled biotin. J Nucl Med.